# Fluorinated and iodinated (Z)-2-(4-(2-fluoroethoxy)benzylidene)-5-iodobenzofuran-3(2H)-one

Chemical name: | Fluorinated and iodinated (Z)-2-(4-(2-fluoroethoxy)benzylidene)-5-iodobenzofuran-3(2H)-one | [image]
Abbreviated name: | [^125^I]3, [^18^F]3 | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | β-amyloid (Aβ) | [image]
Target Category: | Accepters | [image]
Method of detection: | Single-photon emission computed tomography (SPECT), positron emission tomography (PET) | [image]
Source of signal / contrast: | ^125^I, ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents; - Humans | Structures of [^125^I]3 and [^18^F]3 by Watanabe et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=molecular%20imaging%20and%20Alzheimer%u2019s%20disease%20and%20%u03B2-amyloid%20)]

Fluorinated and iodinated (Z)-2-(4-(2-fluoroethoxy)benzylidene)-5-iodobenzofuran-3(2H)-one (compound 3), abbreviated as [^18^F]3 and [^125^I]3, respectively, is an aurone derivative synthesized by Watanabe et al. for single-photon emission computed tomography (SPECT) and positron emission tomography (PET) of Alzheimer’s disease (AD) by targeting β-amyloid (Aβ) plaques (1).

AD is characterized in pathology by the presence of extracellular Aβ plaques, intraneuronal neurofibrillary tangles, and neuronal loss in the cerebral cortex (2, 3). Of them, Aβ deposit is the earliest neuropathological marker and is relatively specific to AD and closely related disorders. Aβ plaques are composed of abnormal paired helical filaments 5–10 nm in size. These filaments are largely made of insoluble Aβ peptides that are 40 or 42 amino acids in length (4).

In recent years, molecular imaging by targeting the extracellular Aβ has been intensively investigated in attempts to detect early AD, assess Aβ content in vivo, determine the timing of anti-plaque therapy, and evaluate the therapeutic efficacy (4). Radiolabeled Aβ40 peptides were tested first, but they showed poor penetration ability to cross the blood–brain barrier (BBB) (4). Based on the fact that Aβ can be specifically stained in vitro with dyes of Congo red, chrysamine G, and thioflavin-T, an effort was made to develop imaging agents with these dyes. This effort, however, was in general unsuccessful because the bulky ionic groups of heteroatoms in these dyes prevent them from crossing the BBB (2). Importantly, a large class of derivatives (e.g., aminonaphthalenes, benzothiazoles, stilbenes, and imidazopyridines) was synthesized with these dyes as templates (4). Clinical and preclinical studies have shown that these derivatives not only possess a high binding affinity with Aβ plaques as their parent compounds, but also exhibit good penetration ability through the BBB and rapid washout from brain.

Ono et al. first synthesized a class of radioiodinated flavone derivatives that present a high binding affinity with Aβ plaques and good penetration ability through the BBB (5). However, these flavone derivatives display poor clearance from the brain, which leads to a high brain background. The investigators then explored another class of flavonoids with aurone as the core structure (6, 7). Aurone is a heterocyclic chemical compound that contains a benzofuran element associated with a benzylidene linked in position 2 and a chalcone-like group being closed into a five-member ring. The aurone derivatives possess a nucleophilic group (NH_2_, NHMe, or NMe_2_) at the 4' position and a radioiodine at the 5 position. Although these aurone derivatives exhibit a strong binding affinity with Aβ (inhibition constant (K_i_) = 1.2–6.8 nM), high penetration ability through the BBB (1.9%−4.6% injected dose per gram tissue (ID/g) at 2 min), and a fast washout from the brain (0.3%−0.5% ID/g at 30 min), the pharmacokinetics of these compounds are less favorable for brain imaging than the pharmacokinetics of the agent [^123^I]IMPY (6-iodo-2-(4'-dimethylamino)phenyl-imidazo[1,2]pyridine), which is the only SPECT agent to be tested in humans to date (1, 8, 9). The investigators also modified the flavone and aurone derivatives by pegylating them with 1–3 units of ethylene glycol at the 4' position or by conjugating them with the chelating agent bis-amino-bis-thiol (BAT) (7). Favorable pharmacokinetics for brain imaging was observed for the pegylated derivatives ([^18^F]8(a–c)) but not for the BAT-chelated derivatives ([^99m^Tc]BAT-FL and [^99m^Tc]BAT-AR) (6, 7).

This series of chapters summarizes the data obtained with flavone and aurone derivatives, including [^125^I]15, [^125^I]9, [^125^I]14, [^125^I]16, [^125^I]17, [^99m^Tc]BAT-FL, [^99m^Tc]BAT-AR, [^18^F]8(a-c), [^125^I]3, and [^18^F]3 (1, 6-8). This chapter presents the data obtained with [^125^I]3 and [^18^F]3 (1).

### Related Resource Links:

- Amyloid-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=amyloid+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)
- Amyloid-targeted imaging clinical trials in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=amyloid)
- Structures and other information of amyloid peptides in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=amyloid)
- Alzheimer’s disease articles in Online Mendelian Inheritance in Man (http://www.ncbi.nlm.nih.gov/omim/?term=Alzheimer%27s%20disease)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21920750)]

Compound 3 was prepared by the reaction of 5-iodobenzofuran-3(2H)-one with 4-(2-fluoroethoxy)benzaldehyde in the presence of Al_2_O_3_ in chloroform at room temperature (yield = 27%) (1). Its tributyltin derivative ((Z)-2-(4-(2-fluoroethoxy)benzylidene)-5-(tributylstannyl)benzofuran-3(2H)-one) was prepared using a halogen-to-tributyltin exchange reaction catalyzed by Pd(0) (yield = 32.2%). The tributyltin derivative was used for radioiodination to prepare [^125^I]3. To prepare [^18^F]3, 5-iodobenzofuran-3(2H)-one was first reacted with 4-(2-hydroxyethoxy)benzaldehyde in the presence of Al_2_O_3_ in chloroform at room temperature to form (Z)-2-(4-(2-hydroxyethoxy)benzylidene)-5-iodobenzofuran-3(2H)-one (compound 5; yield = 48%). The free OH groups of compound 5 were then converted into a tosylate (Ts) by reacting with TsCl in the presence of pyridine to produce (Z)-2-(4-(2-tosyloxyethoxy)benzylidene)-5-iodobenzofuran-3(2H)-one (compound 6), which was used as the precursor to prepare [^18^F]3. The radiochemical identities of [^125^I]3 and [^18^F]3 were verified with high-performance liquid chromatography (HPLC).

The radiochemical yields of both [^125^I]3 and [^18^F]3 were >23%, and their radiochemical purities were >95% after purification with HPLC. [^125^I]IMPY was also prepared as a competing radioligand using the standard iododestannylation reaction. [^125^I]IMPY had a radiochemical purity of >95%. The theoretical specific activities of [^125^I]3 and [^125^I]IMPY were anticipated to be similar to that of ^125^I (81.4 TBq/mmol (2,200 Ci/mmol)) with no-carrier-added preparation. No data for measured specific activities of [^125^I]3, [^18^F]3, and [^125^I]IMPY were reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21920750)]

The binding affinity of compound 3 was measured with Aβ(1−42) aggregates; [^125^I]IMPY was used as the competing radioligand (1). The measurement showed a K_i_ value of 6.81 nM. The octanol/buffer partition coefficient (log P) of [^125^I]3 was measured to be 2.45 ± 0.04. The log P value of [^18^F]3 was not reported.

The binding of unradiolabeled compound 3 with mouse Aβ plaques was confirmed in brain sections of double transgenic AD mice (Tg2576) with fluorescent staining (1). Amyloid plaques were clearly stained with compound 3, and the labeling pattern was consistent with that observed with thioflavin S staining. These results suggest that compound 3 can specifically bind with Aβ plaques in the mouse brain.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21920750)]

The biodistribution of [^125^I]3 and [^18^F]3 was tested in normal mice (n = 5–6 mice/time point for each agent) (1). The initial brain uptake of [^125^I]3 was 2.34% ID/g at 2 min, and the agent was then rapidly eliminated (0.19% ID/g at 60 min after injection). [^18^F]3 showed an initial uptake of 3.66% ID/g at 2 min and rapid clearance from brain, with 1.75% ID/g at 60 min after injection. Although [^125^I]3 and [^18^F]3 displayed some difference in brain uptake, these results suggest that [^125^I]3 and [^18^F]3 may function as a PET/SPECT probes for detecting Aβ plaques in the AD brain.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21920750)]

Postmortem brain tissues from an autopsy-confirmed case of AD and a control subject were used to analyze the binding of [^125^I]3 with human Aβ plaques in brain sections with autoradiography (1). Autoradiographic images showed high levels of radioactivity in the brain sections, and the hot spots of [^125^I]3 were consistent with those of in vitro immunohistochemical staining in the same brain sections. Normal human brain displayed no remarkable accumulation of [^125^I]3. These results demonstrate the feasibility of using [^125^I]3 as a SPECT probe for detecting Aβ plaques in the brains of AD patients. No data were reported for the binding of [^18^F]3 with human Aβ plaques.

## References

1 Watanabe H., Ono M., Kimura H., Kagawa S., Nishii R., Fuchigami T., Haratake M., Nakayama M., Saji H. (2011). A dual fluorinated and iodinated radiotracer for PET and SPECT imaging of beta-amyloid plaques in the brain. Bioorg Med Chem Lett.
2 Ono M. (2009). Development of positron-emission tomography/single-photon emission computed tomography imaging probes for in vivo detection of beta-amyloid plaques in Alzheimer's brains. Chem Pharm Bull (Tokyo).
3 Mathis C.A., Wang Y., Klunk W.E. (2004). Imaging beta-amyloid plaques and neurofibrillary tangles in the aging human brain. Curr Pharm Des.
4 Vallabhajosula S. (2011). Positron emission tomography radiopharmaceuticals for imaging brain Beta-amyloid. Semin Nucl Med.
5 Ono M., Maya Y., Haratake M., Ito K., Mori H., Nakayama M. (2007). Aurones serve as probes of beta-amyloid plaques in Alzheimer's disease. Biochem Biophys Res Commun.
6 Ono M., Watanabe R., Kawashima H., Kawai T., Watanabe H., Haratake M., Saji H., Nakayama M. (2009). 18F-labeled flavones for in vivo imaging of beta-amyloid plaques in Alzheimer's brains. Bioorg Med Chem.
7 Ono M., Ikeoka R., Watanabe H., Kimura H., Fuchigami T., Haratake M., Saji H., Nakayama M. (2010). 99mTc/Re complexes based on flavone and aurone as SPECT probes for imaging cerebral beta-amyloid plaques. Bioorg Med Chem Lett.
8 Maya Y., Ono M., Watanabe H., Haratake M., Saji H., Nakayama M. (2009). Novel radioiodinated aurones as probes for SPECT imaging of beta-amyloid plaques in the brain. Bioconjug Chem.
9 Newberg A.B., Wintering N.A., Plossl K., Hochold J., Stabin M.G., Watson M., Skovronsky D., Clark C.M., Kung M.P., Kung H.F. (2006). Safety, biodistribution, and dosimetry of 123I-IMPY: a novel amyloid plaque-imaging agent for the diagnosis of Alzheimer's disease. J Nucl Med.